# ^64^Cu-Labeled 1,4,7,10-Tetraazacyclododedane-N,N’,N’’,N’’’-tetraacetic acid–conjugated vascular endothelial growth factor A isoform 121-gelonin fusion protein

Chemical name: | ^64^Cu-Labeled 1,4,7,10-Tetraazacyclododedane-N,N’,N’’,N’’’-tetraacetic acid–conjugated vascular endothelial growth factor A isoform 121-gelonin fusion protein
Abbreviated name: | ^64^Cu-DOTA-VEGF_121_/rGel
Synonym:
Agent Category: | Proteins
Target: | Vascular endothelial growth factor receptor (VEGFR)
Target Category: | Receptors
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | Copper-64 (^64^Cu)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=antiangiogenic%20therapy%20and%20VEGFR%20and%20VEGF)]

^64^Cu-Labeled 1,4,7,10-tetraazacyclododedane-N,N’,N’’,N’’’-tetraacetic acid (DOTA)–conjugated vascular endothelial growth factor A isoform 121 (VEGF_121_)-gelonin fusion protein (VEGF_121_/rGel), abbreviated as ^64^Cu-DOTA-VEGF_121_/rGel, is an imaging agent developed by Hsu et al. for monitoring the targeting efficiency and treatment efficacy of the VEGF_121_/rGel immunotoxin (1).

VEGFs are a group of five potent inducers of cell migration, invasion, vascular permeability, and neovascular formation (2). They act via three receptor tyrosine kinases: VEGFR-1, VEGFR-2, and VEGFR-3 (3). These receptors are overexpressed on the endothelial cells of tumor neovasculature and are almost undetectable in the endothelium of adjacent normal tissues. The critical role of the VEGF/VEGFR signal pathway in tumor angiogenesis has prompted great efforts in the development of antiangiogenic therapies, and agents have been tested by acting on different steps of the pathway, such as by binding to the VEGF ligand, inhibiting VEGFR tyrosine kinase, inhibiting downstream effectors (mammalian target of rapamycin inhibitors), and modulating VEGF production (4-6). These agents are highly effective against tumor growth in animal models when they are used alone; however, they seldom lead to tumor regression and exhibit insufficient efficacy in the clinical setting, although combination with chemotherapy has been shown to improve patient survival in certain tumor types. The most likely explanation for this phenominon is that tumor endothelial cells can adapt to antiangiogenic treatment and form functional vasculature that loses sensitivity to the inhibitors of VEGF/VEGFR (4, 6). It is hypothesized that VEGF/VEGFR-targeted therapy should be administrated before the development of a well-established vascular network.

Molecular imaging provides a means to reveal the mechanism underlying this phenomenon and to monitor the antiangionic therapy (1, 7). VEGF_121_/rGel has been generated with VEGF_121_, which is linked with recombinant plant toxin gelonin through a G_4_S tether (4, 8-10). Gelonin is a member of the ribosome-inactivating protein family, which depurinates rRNA and other polynucleotide substrates and subsequently inhibits protein synthesis (11). A series of preclinical studies showed that VEGF_121_/rGel could specifically inhibit the growth of tumor endothelial cells (8-10, 12). Like other immunotoxins, VEGF_121_/rGel is also expected to be effective against tumors resistant to VEGF/VEGFR-targeting inhibitors if the tumor cells express sufficient levels of VEGFR (11). To monitor the VEGFR-targeting efficiency of VEGF_121_/rGel with imaging techniques, Hsu et al. and Cho et al. labeled the VEGF_121_/rGel with ^64^Cu (^64^Cu-DOTA-VEGF_121_/rGel) and with MnFe_2_O_4_ nanoparticles (VEGF_121_/rGel-MNPs), respectively (1, 7). Both imaging studies have concluded that noninvasive imaging with VEGF_121_/rGel will be useful to monitor the treatment efficacy and to identify patients who may benefit from the VEGF_121_/rGel therapy. This chapter summarizes data obtained with ^64^Cu-DOTA-VEGF_121_/rGel (1).

### Related Resource Links:

VEGF/VEGFR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=VEGFR%20AND%20micad%5bbook%5d)

Articles on VEGF in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=vascular%20endothelial%20growth%20factor)

VEGF-related compounds in PubChem Substance (http://www.ncbi.nlm.nih.gov/pcsubstance?term=vascular%20endothelial%20growth%20factor)

VEGF-related nucleotide sequences (http://www.ncbi.nlm.nih.gov/nuccore?term=VEGF)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/17332623)]

Hsu et al. described the synthesis of ^64^Cu-DOTA-VEGF_121_/rGel (1). The synthesis, expression, and purification of the VEGF_121_/rGel immunotoxin were performed as described previously by Veenendaal et al. (8). The molecular weight of VEGF_121_/rGel was 84 kDa. VEGF_121_/rGel was conjugated to DOTA to generate DOTA-VEGF_121_/rGel. Labeling with ^64^Cu was completed in the reaction of ^64^CuCl_2_ and DOTA-VEGF_121_/rGel for 1 h at 40°C.

The total time for ^64^Cu-labeling of the DOTA-VEGF_121_/rGel, including the final purification, was 90 ± 10 min (n = 3). The radiolabeling yield was 85.2 ± 9.2% on the basis of 37 MBq (1 mCi) ^64^Cu per 25 µg DOTA-VEGF_121_/rGel (n = 3). The specific activity of ^64^Cu-DOTA-VEGF_121_/rGel was 1.3 ± 0.1 GBq/mg (35.14 ± 2.7 mCi/mg), and the radiochemical purity was ≥98%. The number of DOTA molecules per VEGF_121_/rGel molecule was 3.3 ± 0.1 (n = 4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/17332623)]

A cell-binding assay with VEGF_121_/rGel and the DOTA-VEGF_121_/rGel conjugate was performed with ^125^I-VEGF_165_ (specific activity, 74 TBq/mmol (2 kCi/mmol)) as the radioligand (1). Both VEGF_121_/rGel and DOTA-VEGF_121_/rGel without the metal inhibited the ^125^I-VEGF_165_ binding to PAE/KDR cells (porcine aortic endothelial cells transfected with cDNA of VEGFR2) in a dose-dependent manner. The 50% inhibition concentrations of VEGF_121_/rGel and DOTA-VEGF_121_/rGel were 24.5 nM and 40.6 nM, respectively, indicating that DOTA conjugation induced no significant change in the VEGF_121_/rGel binding affinity. Western blot analysis (functional assay) of the VEGFR2 expression on PAE/KDR cells revealed a slight decrease in the expression level of phosphorylated VEGFR2 after DOTA conjugation. Increased expression levels of the phosphorylated VEGFR2 were observed at concentrations ≥5 nM for both VEGF_121_/rGel and DOTA-VEGF_121_/rGel.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/17332623)]

Positron emission tomography with ^64^Cu-DOTA-VEGF_121_/rGel was performed in athymic nude mice bearing intracranial tumors (n = 3) (1). Tumors were generated by intracranial injection into the right frontal lobe with 10^5^ firefly luciferase-transfected U87MG human glioblastoma cells (U87MG-fLuc). The mice were intravenously injected with 5–10 MBq (0.14–0.27 mCi) ^64^Cu-DOTA-VEGF_121_/rGel and were imaged for up to 48 h after injection.

^64^Cu-DOTA-VEGF_121_/rGel exhibited high tumor accumulation and retention, as well as high tumor/background contrast from 1 h to 48 h after injection (1). Tumor accumulation at 1 h after injection was 5.8 ± 0.5% injected dose per gram (ID/g) (n = 3) and steadily increased, peaking at ~18 h after injection (11.8 ± 2.3% ID/g). At 46 h after injection, tumor uptake decreased to 8.4 ± 1.7% ID/g. There was no clear relationship between tumor size and tracer uptake. ^64^Cu-DOTA-VEGF_121_/rGel was cleared through both the hepatic and the renal pathways (data not shown). However, no evidence about the in vivo stability of this agent was reported.

A blocking study was carried out by injecting 200 µg VEGF_121_ before injecting ^64^Cu-DOTA-VEGF_121_/rGel. Blocking with VEGF_121_ resulted in a significant reduction in the ^64^Cu-DOTA-VEGF_121_/rGel uptake (P < 0.05), suggesting VEGFR-specific tumor uptake of the ^64^Cu-DOTA-VEGF_121_/rGel (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Hsu A.R., Cai W., Veeravagu A., Mohamedali K.A., Chen K., Kim S., Vogel H., Hou L.C., Tse V., Rosenblum M.G., Chen X. (2007). Multimodality molecular imaging of glioblastoma growth inhibition with vasculature-targeting fusion toxin VEGF121/rGel. J Nucl Med.
2 Koch S., Tugues S., Li X., Gualandi L., Claesson-Welsh L. (2011). Signal transduction by vascular endothelial growth factor receptors. Biochem J.
3 Press M.F., Lenz H.J. (2007). EGFR, HER2 and VEGF pathways: validated targets for cancer treatment. Drugs.
4 Backer M.V., Hamby C.V., Backer J.M. (2009). Inhibition of vascular endothelial growth factor receptor signaling in angiogenic tumor vasculature. Adv Genet.
5 Munagala R., Aqil F., Gupta R.C. (2011). Promising molecular targeted therapies in breast cancer. Indian J Pharmacol.
6 Thorpe P.E. (2004). Vascular targeting agents as cancer therapeutics. Clin Cancer Res.
7 Cho E.J., Yang J., Mohamedali K.A., Lim E.K., Kim E.J., Farhangfar C.J., Suh J.S., Haam S., Rosenblum M.G., Huh Y.M. (2011). Sensitive Angiogenesis Imaging of Orthotopic Bladder Tumors in Mice Using a Selective Magnetic Resonance Imaging Contrast Agent Containing VEGF121/rGel. Invest Radiol.
8 Veenendaal L.M., Jin H., Ran S., Cheung L., Navone N., Marks J.W., Waltenberger J., Thorpe P., Rosenblum M.G. (2002). In vitro and in vivo studies of a VEGF121/rGelonin chimeric fusion toxin targeting the neovasculature of solid tumors. Proc Natl Acad Sci U S A.
9 Mohamedali K.A., Kedar D., Sweeney P., Kamat A., Davis D.W., Eve B.Y., Huang S., Thorpe P.E., Dinney C.P., Rosenblum M.G. (2005). The vascular-targeting fusion toxin VEGF121/rGel inhibits the growth of orthotopic human bladder carcinoma tumors. Neoplasia.
10 Akiyama H., Mohamedali K.A. (2005). E.S. RL, S. Kachi, J. Shen, C. Hatara, N. Umeda, S.F. Hackett, S. Aslam, M. Krause, H. Lai, M.G. Rosenblum, and P.A. Campochiaro, Vascular targeting of ocular neovascularization with a vascular endothelial growth factor121/gelonin chimeric protein. Mol Pharmacol.
11 Wahl, O., M. Oswald, L. Tretzel, E. Herres, J. Arend, and T. Efferth, Inhibition of Tumor Angiogenesis by Antibodies, Synthetic Small Molecules and Natural Products. Curr Med Chem, 2011
12 Ran S., Mohamedali K.A., Luster T.A., Thorpe P.E., Rosenblum M.G. (2005). The vascular-ablative agent VEGF(121)/rGel inhibits pulmonary metastases of MDA-MB-231 breast tumors. Neoplasia.